# ^177^Lu-Labeled h-R3 (nimotuzumab), a humanized monoclonal antibody targeting the external domain of the epidermal growth factor receptor

Chemical name: | ^177^Lu-Labeled h-R3 (nimotuzumab), a humanized monoclonal antibody targeting the external domain of the epidermal growth factor receptor
Abbreviated name: | [^177^Lu]-h-R3
Synonym: | [^177^Lu]-Nimotuzumab
Agent Category: | Antibody
Target: | Epidermal growth factor receptor
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^177^Lu
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=EGFR&cmd=DetailsSearch)]

The epidermal growth factor receptor (EGFR) is a 170-kDa transmembrane protein that promotes cell proliferation through a receptor-associated tyrosine kinase (TK)–mediated signal transduction pathway and is known to participate in the development, survival, and migration of normal cells and a variety of cancerous cells (1). In addition, overexpression of the EGFR in malignant tumors appears to correlate with a poor prognostic outcome for the patient (1). In an effort to develop therapies against cancer, a variety of anti-EGFR monoclonal antibodies (mAbs) that inhibit activation of the receptor (see Di Fede et al. (2) for details) or small molecules that interfere with stimulation of the receptor TK pathway (for details, see Kumar et al. (3)) have been developed and approved by the United States Food and Drug Administration for use in the clinic.

Vallis et al. developed ior egf/r3, a murine mAb with a high affinity for the extracellular domain of the EGFR, labeled it with 99m-technetium, and used it for the molecular imaging of the receptor (4). However, because of immunogenicity, the ^99m^Tc-labeled mAb was considered to have limited clinical application, particularly for patients who required repeated imaging investigations. To alleviate this problem, a humanized ior egf/r3 was developed by combining the complementary determining regions of the murine antibody with a human immunoglobulin-1 framework, and this new agent was designated as h-R3 or nimotuzumab (5). Subsequently, ^99m^Tc-labeled h-R3 was investigated for its tissue distribution and imaging properties in clinical trials using single-photon emission computed tomography (SPECT) (4, 5). From these studies, the investigators concluded that ^99m^Tc-h-R3 can be used for the detection of tumors that overexpress EGFR, but it showed a high accumulation in the liver and kidneys of the patients. In another clinical study, the biodistribution of ^188^Re-labeled h-R3 was investigated with SPECT in patients with high-grade gliomas (http://cancer.gov/dictionary?CdrID=45700) after locoregional administration; it was shown that this mode of administration of ^188^Re-h-R3 was safe and that the radiolabeled mAb could be used for the treatment of this malignancy (6). In a continued effort to develop a radioimmunotherapeutic agent that can be used in the clinic for the radioimmunotherapy of cancerous tumors that overexpress the EGFR, Beckford Vera et al. produced ^177^Lu-labeled h-R3 and investigated its biodistribution in healthy mice and mice bearing A431 human cell epithelial carcinoma xenograft tumors (7).

### Related Resource Links

Chapters on anti-EGFR antibodies (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=EGFR+AND+micad%5Bbook%5D&doptcmdl=TOCView&log%24=booksrch&bname=micad) in MICAD

Protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/NM_005228.3) of human EGFR variant 1

EGFR in OMIM (http://www.ncbi.nlm.nih.gov/omim/131550) (Online Mendelian Inheritance in Man)

EGFR signaling pathways (http://pid.nci.nih.gov/search/pathway_landing.shtml?pathway_id=200086&source=NATURE&what=graphic&jpg=on) (NCI-Nature Pathways Interaction Database)

Anti-EGFR antibodies (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-EGFR%20antibodies&cmd=DetailsSearch) in PubMed

EGFR tyrosine kinase inhibitors (http://www.ncbi.nlm.nih.gov/pubmed?term=egfr%20tyrosine%20kinase%20inhibitors&cmd=DetailsSearch) in PubMed

Clinical trials (http://clinicaltrials.gov/ct2/results?term=EGFR) related to EGFR

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=177Lu%20h-R3%20synthesis&cmd=DetailsSearch)]

h-R3 was purchased from a commercial source and conjugated with either S-2-(4-isothiocyanatobenzyl)-1,4,7,10-tetraazacyclododecane tetraacetic acid (p-SCN-Bn-DOTA) or the acyclic ligand S-2-(4-isothiocyanatobenzyl)-diethylenetriamine pentaacetic acid (p-SCN-Bn-DTPA) for conjugation with ^177^Lu as described by Beckford Vera et al. (7). When a 20:1 ratio of p-SCN-Bn-DOTA or p-SCN-Bn-DTPA was used to produce the conjugates, the average number of chelating groups per molecule of h-R3 was determined to be 4.1 ± 1.3 ([^177^Lu]-(DOTA)_4–5_-h-R3 and [^177^Lu]-(DTPA)_4–5_-h-R3, respectively) (n = 5 experiments). When the conjugation ratio of p-SCN-Bn-DOTA was increased to 50:1, the chelate:h-R3 ratio increased to 7.4 ± 1.5 ( [^177^Lu]-(DOTA)_7–9_-h-R3) (n = 5 experiments).

The radiolabeling yields of ^177^Lu-DOTA-h-R3 and ^177^Lu-DTPA-h-R3 were 99.1 ± 0.5% and 92.3 ± 4.1% (n = 5 determinations for each conjugate), respectively. The radiochemical purities of the purified ^177^Lu-labeled preparations of all the different conjugates were reported to be >98%. The specific activities of [^177^Lu]-(DOTA)_4–5_-h-R3, [^177^Lu]-(DOTA)_7–9_-h-R3, and [^177^Lu]-(DTPA)_4–5_-h-R3 were 673 MBq/6.6 pmol (18.2 mCi/6.6 pmol), 915 MBq/6.6 pmol (24.7 mCi/6.6 pmol), and 478 MBq/6.6 pmol (12.9 mCi/6.6 pmol), respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=21711096%5Buid%5D&cmd=DetailsSearch)]

Using a competitive binding assay with a fixed number of A431 cells and different dilutions of the radioimmunoconjugates, the immunoreactivities of [^177^Lu]-DOTA-h-R3 conjugates and [^177^Lu]-DTPA_4–5_-h-R3 were determined to be 94.5 ± 3.1% and 88.3 ± 4.6%, respectively (7).

Competitive binding studies in the presence of non-radiolabeled h-R3 revealed that the IC_50_ concentrations for [^177^Lu]-DOTA-h-R3 conjugates and [^177^Lu]-DTPA_4–5_-h-R3 were 34.9 ± 2.7 nmol/L and 44.3 ± 5.1 nmol/L, respectively (7).

From saturation binding experiments, the K_d_ values of [^177^Lu]-(DOTA)_4-5_-h-R3 and [^177^Lu]-DTPA_4–5_-h-R3 were determined to be 13.8 ± 1.9 × 10−^8^ mol/L and 12.2 ± 1.3 × 10−^8^ mol/L, respectively (7). The number of binding sites per A431 cell was calculated to be ~2 × 10^6^ from the B_max_ value.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=177Lu-nimotuzumab%20rodentia&cmd=DetailsSearch)]

The biodistribution of the various [^177^Lu]-h-R3 conjugates was studied in normal Balb/c nu/nu mice (n = 3–4 animals/time point) as described by Beckford Vera et al. (7). Little difference in the accumulation of radioactivity from the two ^177^Lu-DOTA-h-R3 conjugates was observed in the blood, but at all the time points a significantly higher amount of label (P < 0.001–0.05) from [^177^Lu]-(DOTA)_4–5_-h-R3 was observed in circulation compared with that from either [^177^Lu]-(DOTA)_7–9_-h-R3 or [^177^Lu]-(DTPA)_4–5_-h-R3. At all time points (24, 72, 96, 168, 216 and 264 h postinjection (p.i.)), the liver showed a significantly higher (P < 0.01) uptake of radioactivity from [^177^Lu]-(DOTA)_7-9_-h-R3 compared with the other two conjugates. Other organs (brain, heart, lungs, kidneys, bone, and stomach) showed almost no difference in uptake of the tracer from all the [^177^Lu]-h-R3 conjugates. Because a higher yield of [^177^Lu]-(DOTA)_4–5_-h-R3 compared to that with [^177^Lu]-(DTPA)_4–5_-h-R3 was obtained during synthesis (>99% versus ~92%) all subsequent studies were performed only with the former ^177^Lu-labeled h-R3 conjugate.

The biodistribution of [^177^Lu]-(DOTA)_4–5_-h-R3 was investigated in mice bearing A431 cell xenograft tumors (7). The animals (n = 4–5 mice/time point) were injected with 150–280 kBq (4.4–7.6 μCi; 66.6 pmol) of the labeled conjugate through the tail vein and euthanized at various time points ranging from 24 h to 264 h p.i. to harvest all the major organs and the tumors. All organs showed a similar trend in uptake and retention of radioactivity from the radiolabeled mAb; maximum uptake was observed at 24 h p.i., and it decreased gradually up to 264 h p.i. The tumor showed a maximum uptake of 22.4 ± 3.1% injected dose per gram tissue (ID/g) at 72 h p.i., which decreased to 18.3 ± 0.3% ID/g by 216 h p.i. and to 12.6 ± 2.8% ID/g at 264 h p.i. The tumor/non-tumor tissue (T/nT) ratios were the highest at 168 h p.i., with reported values of 2.6, 2.4, 6.1, 6.6, 23.5, and 17.5 for blood, liver, spleen, kidneys, muscle, and bone, respectively. See below for results from blocking studies.

In another study, the biodistribution of [^177^Lu]-(DOTA)_4–5_-h-R3 was studied after a locoregional injection of the labeled mAb (i.e., the radiolabeled mAb was injected at the tumor site on the animals) was given to mice (n = 4 animals/time point) bearing A431 cell xenografts (7). The animals were euthanized at different time points ranging from 24 h to 96 h after the injection, and all the major organs, including the tumors, were collected to determine the uptake of radioactivity by the various tissues. In this study, significantly higher uptake of label by the tumors was observed at 24 h and 72 h p.i. compared with the intravenous injection (i.v.) (P < 0.001). The uptake in the lesion peaked to 32.7 ± 2.9% ID/g at 72 h p.i. (compared with 22.4 ± 3.1% ID/g in animals given the i.v. treatment); however, at 96 h p.i. no significant difference in uptake of the label by the tumor (between the i.v. and the locoregional injection) was observed (P > 0.05). At 24 h and 72 h p.i. with the locoregional injection, a significantly lower amount of the tracer was observed in the blood (P < 0.001), liver (P < 0.05), lungs (P < 0.05), and kidneys (P < 0.01) compared with that after the i.v. treatment. After the locoregional injection of [^177^Lu]-(DOTA)_4–5_-h-R3, the T/nT ratios for the blood, liver, spleen, lungs, and kidneys were 4.6, 9.8, 10.5, 9.8, and 11.7 times higher, respectively, than those calculated for the i.v. application. At 72 h p.i., the T/nT ratios mentioned above were two times higher for the locoregional injection than after the i.v. treatment.

In a blocking study, mice bearing A431 cell tumors were injected with [^177^Lu]-(DOTA)_4–5_-h-R3 in the presence of excess non-radiolabeled h-R3 (~67 pmol) (7). At 96 h p.i., the uptake of label by the tumor was significantly lower (6.4 ± 1.8% ID/g) than in mice injected only with the radioimmunoconjugate (18.4 ± 3.3% ID/g and 20.3 ± 2.1% ID/g after i.v. and locoregional injections, respectively).

From these studies, the investigators concluded that [^177^Lu]-(DOTA)_4–5_-h-R3 can be used to target cancerous tumors that overexpress the EGFR; however, further evaluation of the radiolabeled mAb is necessary before it can be used in the clinic (7).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=177Lu-nimotuzumab%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=177Lu-nimotuzumab%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=177Lu-nimotuzumab%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Bronte G., Terrasi M., Rizzo S., Sivestris N., Ficorella C., Cajozzo M., Di Gaudio F., Gulotta G., Siragusa S., Gebbia N., Russo A. (2011). EGFR genomic alterations in cancer: prognostic and predictive values. Front Biosci.
2 Di Fede G., Bronte G., Rizzo S., Cervetto C.R., Cocorullo G., Gulotta G., Bazan V., Russo A. (2011). Monoclonal antibodies and antibody fragments: state of the art and future perspectives in the treatment of non-haematological tumors. Expert Opin Biol Ther.
3 Kumar A., Petri E.T., Halmos B., Boggon T.J. (2008). Structure and clinical relevance of the epidermal growth factor receptor in human cancer. J Clin Oncol.
4 Vallis K.A., Reilly R.M., Chen P., Oza A., Hendler A., Cameron R., Hershkop M., Iznaga-Escobar N., Ramos-Suzarte M., Keane P. (2002). A phase I study of 99mTc-hR3 (DiaCIM), a humanized immunoconjugate directed towards the epidermal growth factor receptor. Nucl Med Commun.
5 Torres L.A., Perera A., Batista J.F., Hernandez A., Crombet T., Ramos M., Neninger E., Perez M., Sanchez E.L., Romero S., Aguilar V., Coca M.A., Iznaga-Escobar N. (2005). Phase I/II clinical trial of the humanized anti-EGF-r monoclonal antibody h-R3 labelled with 99mTc in patients with tumour of epithelial origin. Nucl Med Commun.
6 Torres L.A., Coca M.A., Batista J.F., Casaco A., Lopez G., Garcia I., Perera A., Pena Y., Hernandez A., Sanchez Y., Romero S., Leyva R., Prats A., Fernandez R. (2008). Biodistribution and internal dosimetry of the 188Re-labelled humanized monoclonal antibody anti-epidemal growth factor receptor, nimotuzumab, in the locoregional treatment of malignant gliomas. Nucl Med Commun.
7 Beckford Vera D.R., Eigner S., Henke K.E., Lebeda O., Melichar F., Beran M. (2012). Preparation and preclinical evaluation of (177)Lu-nimotuzumab targeting epidermal growth factor receptor overexpressing tumors. Nucl Med Biol.